# [^18^F]-Fluoro-2-deoxy-D-glucose-folate

Chemical name: | [^18^F]-Fluoro-2-deoxy-D-glucose-folate | [image]
Abbreviated name: | [^18^F]-5 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Folate receptors | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of [^18^F]-5 and [^18^F]-8 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=FDG%20and%20folate%20and%20imaging)]

[^18^F]-Fluoro-2-deoxy-D-glucose ([^18^F]FDG)-folate, abbreviated as [^18^F]-5, is a conjugate of [^18^F]-fluorodeoxyglucose and folate, which was synthesized by al Jammaz et al. for use with positron emission tomography (PET) of tumors by targeting glucose metabolism and folate receptor (1).

2-Deoxy-D-glucose (2DG) was originally synthesized to inhibit glucose utilization by cancer cells and was later labeled with ^18^F for imaging purposes (2, 3). [^18^F]FDG, like glucose, is transported into cells by glucose transporters and converted to [^18^F]FDG-6-phosphate ([^18^F]FDG-6-P) within cells. Because [^18^F]FDG-6-P cannot be further metabolized, it is then trapped within cells. Tumor cells are highly proliferative and have a high rate of glucose metabolism compared to normal tissue. Consequently, tumor cells accumulate much more [^18^F]FDG-6-P than normal cells.

PET imaging with [^18^F]FDG ([^18^F]FDG-PET) has been widely accepted as a standard modality in the detection, staging, and therapy response monitoring of various malignant tumors. However, there are several limitations for the clinical use of [^18^F]FDG-PET (4, 5). First, [^18^F]FDG can accumulate in several important organs, including the brain and heart, which not only limits its use in these organs but also causes toxicity to them. Second, [^18^F]FDG-PET is not suitable for imaging well-differentiated, low-malignant, and slow-growing tumors because these tumors often have low glucose utilization. Third, activated inflammatory cells have been found to take up considerable [^18^F]FDG; thus, false-positivity may become an issue when inflammatory cell infiltrate is prominent in tumors or other diseases.

In an effort to develop new [^18^F]FDG-based imaging probes, al Jammaz et al. synthesized two conjugates, [^18^F]-5 and [^18^F]-8, by conjugating [^18^F]FDG with folate and methotrexate (MTX), respectively, using the readily available oxime-reactive [^18^F]FDG building block (1). Folate is vital for the rapid proliferation of tumor cells, and folate receptor is highly affinitive and overexpressed in various types of human tumors (6, 7). In contrast, healthy cells are severely restricted in possessing folate receptors. In addition, folate conjugates have well been characterized as drugs, drug carriers, and imaging agents (8, 9). MTX is a folic acid analog but possesses a relatively low affinity for folate receptor. Studies by al Jammaz et al. showed that [^18^F]-5 was more suitable for tumor imaging than [^18^F]-8 (1). This chapter summarizes the data obtained with [^18^F]-5 and [^18^F]-8.

### Related Resource Links:

- Folate-based chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD
- Folate receptor gene (http://www.ncbi.nlm.nih.gov/gene/2348) information in NCBI
- Folate receptor-related (http://www.ncbi.nlm.nih.gov/omim?term=folate%20receptor) articles in Online Mendelian Inheritance in Man (OMIM)
- Folate receptor-associated clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor&Search=Search)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22445744)]

The amide-linked reference compounds 5 (2-fluoro-2-deoxy-D-glucose-folate) and 8 (2-fluoro-2-deoxy-D-glucose-methotrexate) were synthesized by conjugating FDG with the γ-isomers of folate carbohydrazide oxime and methotrexate carbohydrazide oxime, respectively (1). The overall chemical yields for compounds 5 and 8 were 62% and 38%, respectively, which appeared to decompose beyond 185°C. The calculated molecular mass for compounds 5 and 8 were 692.61 and 705.65, respectively. The base peak m/z = 325 corresponds to the γ-moiety-(CH_2_-CH_2_-CO-NH-NH-oxime-FDG) of the conjugated folic acid and MTX. Chemical purities for both 5 and 8 were found to be >97%.

[^18^F]-5 and [^18^F]-8 were prepared by reacting the building block of [^18^F]FDG with folate and methotrexate carbohydrazide oximes in acetate buffer (pH ~4.5) for 10–15 min at 60°C (1). The overall radiochemical yields for [^18^F]-5 and [^18^F]-8 were >80% (based on the starting [^18^F]-FDG), with a total synthesis time of ~20 min. The radiochemical purities of [^18^F]-5 and [^18^F]-8 were >98%. The calculated partition coefficients for [^18^F]-5 and [^18^F]-8 were –1.54 ± 0.03 and –1.59 ± 0.02, respectively, representing a low lipophilic characteristic for both conjugates. The amount of cold compounds in the final products was below the detection limit of ultraviolet-visible spectroscopy (<1 µg). The specific activities for [^18^F]-5 and [^18^F]-8 were >9.25 GBq/µmol (250 mCi/μmol). The calculated charged density for [^18^F]-5 was found to be around –1.67, which is 4 and 12 times higher, respectively, than that of the corresponding fluoropyridine and benzene carbohydrazide-folate conjugates (8).

Proteolytic degradation analysis showed that both [^18^F]-5 and [^18^F]-8 remained sufficiently stable (>99%) in human plasma during incubation for at least 4 h at 37°C, demonstrating a high in vitro stability of the two radioconjugates (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22445744)]

The binding affinities (K_d_) of [^18^F]-5 and [^18^F]-8 were evaluated with saturation assays using folate receptor-positive human oral carcinoma KB cell line (1). The results demonstrated that [^18^F]-5 had a higher binding affinity to KB cells than [^18^F]-8 (1.83 ± 0.15 versus 4.74 ± 0.71 nM), comparable to the native folic acid.

Cellular internalization studies were performed with acidic buffer to determine the extent of internalization of [^18^F]-5 and [^18^F]-8 by KB cancer cells (1). A rapid and significant internalization was observed for both [^18^F]-5 and [^18^F]-8, with 25.92 ± 0.59% and 21.50 ± 0.10%, respectively, of the cell surface-bound conjugates internalized after incubation in acidic buffer for 20 min at 37°C, indicating that both conjugates maintained their integrity and displayed high affinity toward folate receptor.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22445744)]

Biodistribution of [^18^F]-5 and [^18^F]-8 was investigated in normal Balb/c mice at 10, 60, and 120 min after tail vein injection (20 µCi, 740 kBq) (n = 4 mice/time points per agent) (1). The results for [^18^F]-5 generally demonstrated fast and efficient clearance from blood and most organs (Table 1). [^18^F]-5 displayed elevated radioactivity uptake and retention in the kidneys and lungs even at 120 min after injection, suggesting that the major route of [^18^F]-5 elimination was the urinary system, which might be attributed to the presence of the hydrophilic [^18^F]-FDG prosthetic group. [^18^F]-8 exhibited almost equal radioactivity accumulation in most organs, and clearance from blood and nearly all organs was fast except for the intestines, where significant radioactivity accumulation was observed. Low bone radioactivity was observed for both [^18^F]-5 and [^18^F]-8. Thus, the high in vivo stability was probably due to the presence of a strong carbon-fluorine bond (1).

Table 1. Biodistribution of [^18^F]-5 and [^18^F]-8 in normal Balb/c mice.

Organs | [^18^F]-5 (% ID/g) | | | [^18^F]-8 (% ID/g)
Organs | 10 min | 60 min | 120 min | 10 min | 60 min | 120 min
Blood | 3.26 ± 0.75 | 0.40 ± 0.17 | 0.22 ± 0.04 | 3.06 ± 0.57 | 1.30 ± 0.25 | 0.82 ± 0.21
Liver | 2.85 ± 0.34 | 0.54 ± 0.07 | 0.47 ± 0.14 | 3.58 ± 0.39 | 1.45 ± 0.27 | 0.69 ± 0.16
Lung | 2.24 ± 0.69 | 2.08 ± 0.16 | 1.20 ± 0.13 | 4.02 ± 0.71 | 1.29 ± 0.26 | 0.59 ± 0.14
Kidney | 5.80 ± 1.38 | 1.83 ± 0.16 | 1.03 ± 0.32 | 3.23 ± 0.48 | 1.83 ± 0.55 | 0.78 ± 0.29
Intestine | 2.35 ± 0.69 | 0.78 ± 0.25 | 0.72 ± 0.05 | 2.91 ± 0.59 | 2.56 ± 0.53 | 1.52 ± 0.05
Heart | 3.26 ± 0.90 | 0.69 ± 0.26 | 0.45 ± 0.09 | 5.09 ± 0.92 | 0.91 ± 0.22 | 0.71 ± 0.16
Muscle | 0.76 ± 0.03 | 0.35 ± 0.04 | 0.37 ± 0.06 | 4.71 ± 0.38 | 0.98 ± 0.23 | 0.55 ± 0.20
Bone | 0.83 ± 0.40 | 0.50 ± 0.07 | 0.44 ± 0.18 | 0.93 ± 0.36 | 0.62 ± 0.19 | 0.59 ± 0.18
Spleen | 1.42 ± 0.18 | 0.73 ± 0.25 | 0.83 ± 0.11 | 2.42 ± 0.36 | 1.19 ± 0.33 | 0.81 ± 0.33

In nude mice bearing KB xenograft tumors (n = 4/group), [^18^F]-5 displayed a rapid clearance from blood with 0.30 ± 0.23% injected dose per gram tissue (ID/g) remained at 60 min after injection (Table 2) (1). High tumor uptake was observed for [^18^F]-5 (3.32 ± 0.32% ID/g) at 60 min after injection, and the tumor/blood and tumor/muscle ratios reached 11.07 and 9.22, respectively. Similar to the findings in normal mice, a moderate uptake of [^18^F]-5 was also found in the kidneys (1.49 ± 0.05% ID/g), but this was much lower than the uptake of [^18^F]-fluorobenzene and pyridine carbohydrazide-folate conjugates (19.7 ± 2.25 and 7.90 ± 1.25% ID/g, respectively) reported previously (8). The relatively low uptake in the kidneys may be attributed to the nature of [^18^F]FDG as a prosthetic group and the overall negative charge for [^18^F]-5. [^18^F]-5 also showed low accumulation in the liver and intestine (0.70 ± 0.61 and 0.75 ± 0.03% ID/g, respectively).

For blocking studies, each animal was intravenously injected with excess cold folic acid (~100 µg) 10 min before injection of the radiotracers (1). Animals were euthanized at 60 min after radiotracer injection (n = 4 mice/group). Cold folic acid markedly reduced the uptake of [^18^F]-5 in the target organs and tumors. [^18^F]-5 uptake was reduced in tumors by ~80% (3.32 ± 0.32 versus 0.72 ± 0.21% ID/g, P < 0.05), indicating receptor specificity of [^18^F]-5. [^18^F]-5 uptake by the kidneys was also considerably reduced by at least 50% (1.49 ± 0.05 versus 0.77 ± 0.05% ID/g, P < 0.05). The radioactivity in other organs either remained at the same degree or increased as observed for the liver and intestine.

Table 2. Biodistribution of [^18^F]-5 and [^18^F]-8 in mice bearing tumor xenografts.

Organs | [^18^F]-5 (% ID/g) | | [^18^F]-8 (% ID/g)
Organs | 60 min | 60 min blocked^a^ | 60 min | 60 min blocked^a^
Blood | 0.30 ± 0.23 | 0.31 ± 0.29 | 0.37 ± 0.17 | 0.22 ± 0.03
Liver | 0.70 ± 0.61 | 1.45 ± 0.30 | 0.61 ± 0.31 | 0.38 ± 0.07
Lung | 1.30 ± 0.30 | 1.49 ± 0.19 | 1.16 ± 0.41 | 1.47 ± 0.21
Kidney | 1.49 ± 0.05 | 0.77 ± 0.05 | 0.82 ± 0.05 | 0.78 ± 0.15
Intestine | 0.75 ± 0.03 | 1.75 ± 0.38 | 0.90 ± 0.25 | 0.88 ± 0.16
Heart | 0.20 ± 0.08 | 0.12 ± 0.04 | 0.21 ± 0.03 | 0.30 ± 0.15
Muscle | 0.36 ± 0.10 | 0.38 ± 0.06 | 0.44 ± 0.05 | 0.52 ± 0.17
Bone | 0.09 ± 0.05 | 0.15 ± 0.02 | 0.16 ± 0.06 | 0.17 ± 0.07
Spleen | 1.30 ± 0.31 | 1.42 ± 0.35 | 1.37 ± 0.35 | 0.83 ± 0.28
Tumor | 3.32 ± 0.32 | 0.72 ± 0.21 | 1.10 ± 0.21 | 0.37 ± 0.33

^a^Animals were injected with 100 μg folic acid 10 min before the administration of radiotracers.

[^18^F]-8 also displayed fast clearance from blood and most of the other organs, but this clearance was slower than that of [^18^F]-5 (Table 2) (1). In addition, [^18^F]-8 exhibited two-fold lower kidney uptake (0.82 ± 0.05% ID/g) and almost four-fold lower tumor uptake (1.1 ± 0.21% ID/g) at 60 min after injection when compared with uptake of [^18^F]-5. Cold folic acid also blocked the uptake of [^18^F]-8 in tumors by ~60% (1.10 ± 0.21 versus 0.37 ± 0.33% ID/g; P < 0.05), suggesting receptor-mediated accumulation of this radioconjugate.

Analysis of the urine collected at 60 min after injection showed that a significant amount of radioactivity (>95%) was still associated with [^18^F]-5 and [^18^F]-8, suggesting that neither radiolabel is prone to rapid in vivo degradation (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Al Jammaz I., Al-Otaibi B., Amer S., Al-Hokbany N., Okarvi S. (2012). Novel synthesis and preclinical evaluation of folic acid derivatives labeled with (18)F-[FDG] for PET imaging of folate receptor-positive tumors. Nucl Med Biol.
2 Laszlo J., Humphreys S.R., Goldin A. (1960). Effects of glucose analogues (2-deoxy-D-glucose, 2-deoxy-D-galactose) on experimental tumors. J Natl Cancer Inst.
3 Fowler J.S. (2002). andIdo, T. Initial and subsequent approach for the synthesis of 18FDG. Semin Nucl Med.
4 Jadvar H. (2011). Prostate cancer: PET with 18F-FDG, 18F- or 11C-acetate, and 18F- or 11C-choline. J Nucl Med.
5 Pery C., Meurette G., Ansquer C., Frampas E., Regenet N. (2010). Role and limitations of 18F-FDG positron emission tomography (PET) in the management of patients with pancreatic lesions. Gastroenterol Clin Biol.
6 Campbell I.G., Jones T.A., Foulkes W.D., Trowsdale J. (1991). Folate-binding protein is a marker for ovarian cancer. Cancer Res.
7 Low P.S. (2009). andKularatne, S.A. Folate-targeted therapeutic and imaging agents for cancer. Curr Opin Chem Biol.
8 Al Jammaz I., Al-Otaibi B., Amer S., Okarvi S.M. (2011). Rapid synthesis and in vitro and in vivo evaluation of folic acid derivatives labeled with fluorine-18 for PET imaging of folate receptor-positive tumors. Nucl Med Biol.
9 Reddy J.A., Allagadda V.M., Leamon C.P. (2005). Targeting therapeutic and imaging agents to folate receptor positive tumors. Curr Pharm Biotechnol.